# ^68^Ga-1,4,7,10-Tetraazacyclododecane-N,N’,N’’,N’’’-1,4,7,10-tetraacetic acid-rhenium-cyclized-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_

Chemical name: | ^68^Ga-1,4,7,10-Tetraazacyclododecane-N,N’,N’’,N’’’-1,4,7,10-tetraacetic acid-rhenium-cyclized-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_
Abbreviated name: | ^68^Ga-DOTA-ReCCMSH(Arg^11^)
Synonym:
Agent category: | Peptide
Target: | Melanocortin-1 (MC-1) receptor, MC1R
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=27477129), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=27477128) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=4157&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about the Melanocortin-1 receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=reCCMSH)]

Malignant melanoma is the most deadly form of skin cancer (1). Early and accurate diagnosis is necessary for surgery and successful treatment (2). The melanocortin (MC) system is a neuropeptide network of the skin, and it is involved in pigmentation regulation, cortisol production, and many other physiological processes (3). Most cutaneous cell types express MC receptors, pro-opiomelanocortin (POMC), and prohormone convertases, and they also release MCs. Melanotropin-stimulating hormones (α-, β-, and γ-MSH) are derived from POMC by the proteolytic action of prohormone convertases. There are five MC receptors (MC1R to MC5R), which belong to the G-protein−coupled receptor superfamily. However, these receptors have been found to be overexpressed in melanoma cells (4, 5). α-MSH (Ac-Ser^1^-Tyr^2^-Ser^3^-Met^4^-Glu^5^-His^6^-Phe^7^-Arg^8^-Trp^9^-Gly^10^-Lys^11^-Pro^12^-Val^13^-NH_2_), produced by the brain and pituitary gland, is a tridecapeptide (13 amino acids) and is the most potent melanotropic peptide (6) in the regulation of skin pigmentation via the MC1R.

Although positron emission tomography (PET) imaging with [^18^F]fluoro-2-deoxy-2-D-glucose ([^18^F]FDG) is effective in the detection of melanoma, it is not melanoma-specific and some melanoma cells do not take up [^18^F]FDG (7, 8). Radiolabeled α-MSH peptide analogs have been shown to specifically bind to MC1R that is overexpressed on human and mouse melanoma cells (4, 5, 7, 9, 10). 1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) has been successfully coupled to the α-MSH peptide analogs for radiolabeling with a variety of radionuclides (7). To improve the tumor/kidney uptake ratio and metabolic stability, a rhenium-cyclized α-MSH analog, Re-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_ (Re-CCMSH(Arg^11^)), was conjugated with DOTA. DOTA-Re-CCMSH(Arg^11^) was radiolabeled with ^68^Ga as a potential molecular imaging agent to target melanoma. ^68^Ga is a positron emitter with a physical half-life of 68 min and is suitable for PET imaging.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=reCCMSH+and+synthesis)]

Wei et al. (11) reported the synthesis of ^68^Ga-DOTA-ReCCMSH(Arg^11^). The DOTA-CCMSH(Arg^11^) peptide was synthesized using standard Fmoc/HBTU(2-[1H-benzotriazole-1-yl]-l,1,3,3,-tetramethyluronium hexafluorophosphate) chemistry on an amide resin with a peptide synthesizer as reported previously by Chen et al. (10). A mixture of DOTA-CCMSH(Arg^11^) and ReOCl_3_ (1:1.5 molar ratio) was incubated for 2 h at 75°C. The cyclized peptide, DOTA-ReCCMSH(Arg^11^), was purified with high-performance liquid chromatography (HPLC). The overall synthetic yield was 10–20%. For ^68^Ga labeling, ^68^GaCl_3_ in 0.1 M hydrochloric acid was added to DOTA-ReCCMSH(Arg^11^) in 1.25 M ammonium acetate, and the mixture was heated for 30 min at 85ºC. Radiochemical purity (as confirmed with HPLC) was >95% with a specific activity of 3.85 TBq/mmol (104 Ci/mmol) and a labeling yield of <10%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=reCCMSH+AND+in+vitro)]

Chen et al. (10) conducted in vitro competitive receptor-binding studies of ReCCMSH and DOTA-ReCCMSH with B16/F1 murine melanoma cells (MC1R-positive). The inhibition concentrations were 2.9 ± 0.3 nM and 1.2 ± 0.3 nM for ReCCMSH and DOTA- ReCCMSH, respectively. The radioactive ligand was ^125^I-Tyr^2^-[Nle^4^,D-Phe^7^]α-MSH.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ReCCMSH+AND+rodentia)]

Wei et al. (11) performed biodistribution studies in female C57BL/6 mice (n = 5/group) bearing 10-day-old B16/F1 murine melanoma tumors. Each mouse received 0.444 MBq (0.012 mCi (~0.1 nmol)) ^68^Ga-DOTA-ReCCMSH(Arg^11^). The radioactivity levels in percent injected dose per gram (% ID/g) were obtained at 30 min and 2 h after injection. The tumor uptake of ^68^Ga-DOTA-ReCCMSH(Arg^11^) was 4.31 ± 1.94% ID/g at 30 min and 4.25 ± 1.41% ID/g at 2 h, indicating that the tumor retention is high. Pre-administration of 10 nmol DOTA-ReCCMSH(Arg^11^) significantly reduced the tumor uptake to 0.42 ± 0.05% ID/g (P <.01) at 2 h after injection. No other tissues showed significant inhibition by DOTA-ReCCMSH(Arg^11^). The nontarget tissue uptake of ^68^Ga-DOTA-ReCCMSH(Arg^11^) was high at 30 min. However, the radioactivity was quickly cleared from all tissues at 2 h after injection (e.g., kidney: 16.50 ± 4.30% ID/g at 30 min and 6.80 ± 1.72% ID/g at 2 h, P < 0.01; blood: 4.65 ± 0.84% ID/g at 30 min and 0.40 ± 0.13% ID/g at 2 h, P < 0.001; liver: 1.34 ± 0.09% ID/g at 30 min and 0.50 ± 0.11% ID/g at 2 h, P < 0.00001). The fast clearance from normal tissues and high tumor retention resulted in good tumor/nontarget tissue ratios at 2 h (e.g., tumor/muscle ratio of 42). When 15 mg L-lysine was coinjected with ^68^Ga-DOTA-ReCCMSH(Arg^11^), the kidney and tumor radioactivity levels were decreased by 53% and 19% at 2 h after injection, respectively. In contrast, the radioactivity levels in other major tissues were not affected. PET imaging of mice bearing the B16/F1 melanomas in the neck was conducted with intravenous injection of 3.7 MBq (0.1 mCi (1 nmol)) ^68^Ga-DOTA-ReCCMSH(Arg^11^) at 0.5, 1, and 2 h. At 0.5 h, the tumor, kidney, blood, lung, and heart were visible. As the background radioactivity decreased, only the tumor, kidney, and bladder were clearly visible by 2 h. Pre-injection of 10 nmol DOTA-ReCCMSH(Arg^11^) inhibited the tumor accumulation of radioactivity by ~50% at all time points, whereas there was little effect on the kidney and liver radioactivity levels.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ReCCMSH+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ReCCMSH+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=reCCMSH+AND+human)]

No publication is currently available.

## NIH Support

R24 CA86307, P50 CA103130, R24 CA86060, P30 CA91842, R41 CA85106

## References

1 Jemal A., Siegel R., Ward E., Murray T., Xu J., Thun M.J. (2007). Cancer statistics, 2007. CA Cancer J Clin.
2 Miao Y., Hylarides M., Fisher D.R., Shelton T., Moore H., Wester D.W., Fritzberg A.R., Winkelmann C.T., Hoffman T., Quinn T.P. (2005). Melanoma therapy via peptide-targeted {alpha}-radiation. Clin Cancer Res.
3 Bohm M., Luger T.A., Tobin D.J., Garcia-Borron J.C. (2006). Melanocortin receptor ligands: new horizons for skin biology and clinical dermatology. J Invest Dermatol.
4 Miao Y., Whitener D., Feng W., Owen N.K., Chen J., Quinn T.P. (2003). Evaluation of the human melanoma targeting properties of radiolabeled alpha-melanocyte stimulating hormone peptide analogues. Bioconjug Chem.
5 Siegrist W., Solca F., Stutz S., Giuffre L., Carrel S., Girard J., Eberle A.N. (1989). Characterization of receptors for alpha-melanocyte-stimulating hormone on human melanoma cells. Cancer Res.
6 Catania A., Airaghi L., Garofalo L., Cutuli M., Lipton J.M. (1998). The neuropeptide alpha-MSH in HIV infection and other disorders in humans. Ann N Y Acad Sci.
7 Weiner R.E., Thakur M.L. (2005). Radiolabeled peptides in oncology: role in diagnosis and treatment. BioDrugs.
8 Dimitrakopoulou-Strauss A., Strauss L.G., Burger C. (2001). Quantitative PET studies in pretreated melanoma patients: a comparison of 6-[18F]fluoro-L-dopa with 18F-FDG and (15)O-water using compartment and noncompartment analysis. J Nucl Med.
9 Tatro J.B., Reichlin S. (1987). Specific receptors for alpha-melanocyte-stimulating hormone are widely distributed in tissues of rodents. Endocrinology.
10 Chen J., Cheng Z., Owen N.K., Hoffman T.J., Miao Y., Jurisson S.S., Quinn T.P. (2001). Evaluation of an (111)In-DOTA-rhenium cyclized alpha-MSH analog: a novel cyclic-peptide analog with improved tumor-targeting properties. J Nucl Med.
11 Wei L., Miao Y., Gallazzi F., Quinn T.P., Welch M.J., Vavere A.L., Lewis J.S. (2007). Gallium-68-labeled DOTA-rhenium-cyclized alpha-melanocyte-stimulating hormone analog for imaging of malignant melanoma. Nucl Med Biol.